# (4S)-4-(3-[^18^F]Fluoropropyl)-L-glutamate

Chemical name: | (4S)-4-(3-[^18^F]Fluoropropyl)-L-glutamate | [image]
Abbreviated name: | [^18^F]FSPG | [image]
Synonym: | [^18^F]BAY 94-9392 | [image]
Agent Category: | Compound | [image]
Target: | x_c_− transporter (sodium-independent anionic amino acid transport system specific for cysteine and glutamate) | [image]
Target Category: | Transporter | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Humans | Structure of [^18^F]FSPG

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=BAY%2094-9392&cmd=DetailsSearch)]

The cystine (dimer of L-cysteine)/glutamate antiporter system x_c_− is a heterodimeric, sodium-independent, and chloride-dependent anionic amino acid (aa) transporter that transports cystine out of the cell and glutamate into the cell at a ratio of 1:1 (1). In general, the cystine concentration within the cell is very low (because intracellular cystine is rapidly cleaved into two molecules of L-cysteine), and the intracellular concentration of glutamate is relatively higher than in the extracellular spaces. Cysteine is not only a component of most proteins; it is also required for the synthesis of glutathione (GSH; a L-γ-glutamyl-L-cysteinyl-glycine tripeptide), an important detoxifier that scavenges and reduces the reactive oxygen or nitrogen species (RO/NS) generated during the metabolic activity of cells (the RO/NS are known to oxidize and denature or modify the activity of proteins, lipids, and DNA in a cell) (2). In addition, GSH influences the intracellular redox signaling pathways during the progression of cell death (2). Therefore, system x_c_− is believed to play an important role in regulating the concentration of GSH in a cell and plays an important role in several physiological processes, such as immune response, inflammation, cellular infection by oncogenic Kaposi’s sarcoma herpesvirus, pathogenesis of disorders of the eye (such as age-related macular degeneration) and central nervous system (such as Alzheimer's disease, epilepsy, and cerebral ischemia), growth and progression of cancer, and the development resistance to anticancer drugs by neoplastic cells; for a detailed discussion on the roles of system x_c_− and GSH in health and disease, see Lewerenz et al., and Franco and Cidlowski (1, 2). Many cancerous tissues have a survival advantage over normal cells because they show a higher expression of system x_c_−, accumulate above-normal levels of L-cysteine and L-glutamate, and maintain high levels of GSH to detoxify the RO/NS efficiently (3). Therefore, a variety of inhibitors that target the x_c_− antiporter have been evaluated for drug sensitization or the treatment of cancer (3).

Increased growth and proliferation are the typical characteristics of cancer cells. To maintain these processes, the cells have an increased demand for energy, exhibit increased macromolecules, and metabolize D-glucose and L-glutamine to produce elevated amounts of fatty acids and aa that are required for the survival of the tumor cells (4). There are indications that many tumors do not use the glycolytic pathway and metabolize nutrients such as L-glutamine to produce energy (5). [^18^F]-Fluorodeoxyglucose ([^18^F]-FDG), an analog of glucose that is transported into and metabolized similarly to glucose in the cell (after phosphorylation to [^18^F]-FDG-6 phosphate, it cannot be further metabolized by glycolysis and remains metabolically trapped within the cell), is often used to detect, stage, and monitor cancer therapy with positron emission tomography (PET) [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fdg%20cancer&cmd=DetailsSearch)]. However, a major drawback of PET imaging with [^18^F]-FDG is that, in addition to tumor cells, normal cells in the brain, heart, brown adipose tissue, etc., also utilize above-average amounts of glucose for energy generation, which can lead to the generation of false-positive results (6). Moreover, it is known that [^18^F]-FDG imaging cannot always distinguish between infection, inflammation, and tumors (6).

On the basis of the information described above, it was hypothesized that PET agents that target system x_c_− can probably be used to visualize tumors that have an enhanced expression and activity of the antiporter (5). The ^18^F-labeled structural analog of L-glutamate 4-[^18^F]fluoro-L-glutamate (BAY 85-8050) was prepared and evaluated with PET for the visualization of tumors in humans (5). In vitro studies showed that the labeled compound was transported by both system x_c_− and the sodium-dependent glutamate transporters. In humans, the tumors showed some uptake of the label, but suboptimal PET images were obtained because the labeled compound was defluorinated while it was in circulation (5). Koglin et al. proposed that, to visualize tumors that overexpress system x_c_− with PET, it is necessary to have an agent that is not only metabolically stable but should interact specifically with the system x_c_− transporter (5). To test this, several ^18^F-labeled derivatives of L-glutamine were prepared, and it was shown that, among all the ^18^F-labeled compounds that were evaluated, only (4S)-4-(3-[^18^F]fluoropropyl)-L-glutamate ([^18^F]FSPG, [^18^F]BAY 94-9392) was stable in mouse blood and could be used with PET to visualize tumors that overexpress system x_c_− in mice and rats (5). In clinical studies, it was shown that [^18^F]FSPG can be used with PET to visualize non-small cell lung cancer (NSCLC) and breast cancer lesions (7), as well as hepatocellular carcinoma (HCC) tumors (8) in humans.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Glutamine%20transporter%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Amino acid transporters (http://www.ncbi.nlm.nih.gov/books/?term=Amino+acid+transporters+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

x_c_− transporter in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/607933))

Human x_c_− transporter system in Gene Database (http://www.ncbi.nlm.nih.gov/gene/23657). Gene ID: 23657

Protein (http://www.ncbi.nlm.nih.gov/protein/Q9UPY5.1) sequence of human x_c_− transporter

Clinical trials (http://clinicaltrials.gov/ct2/results?term=amino+acid+transporter+&Search=Search) related to amino acid transporters

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DFSPG%20synthesis&cmd=DetailsSearch)]

The synthesis of nonradioactive FSPG and its labeling with ^18^F has been described by Koglin et al. (5). The total time taken to synthesize [^18^F]FSPG was 41–51 min; the radiochemical yield (RCY) and radiochemical purity (RCP) of the final product were 40%–63% and >92%, respectively (as determined with radiographic thin-layer chromatography (TLC; R_f_ = 0.46) and high-performance liquid chromatography). The RCP, RCP, and specific activity of [^18^F]FSPG used in a clinical study were reported to be 29.1 ± 5.0%, 90.8 ± 0.5%, and >18.2 GBq/μmol (~0.5 Ci/μmol), respectively (7). In another publication, the specific activity of [^18^F]FSPG at the end of synthesis was reported to be 65.3 ± 15.6 GBq/μmol (1.17 ± 0.42 Ci/μmol) (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DFSPG%20in%20vitro%20studies&cmd=DetailsSearch)]

Using competition assays with NIH-H460 lung cancer cells, the IC_50_ values of non-radioactive FSPG against [^3^H]L-glutamine and [^3^H]L-cysteine, the natural radiolabeled ligands of system x_c_− transporter, were reported to be 29.1 μmol/L and 33.6 μmol/L, respectively (5). The IC_50_ values for L-glutamine and L-cysteine with these cells were 117.2 μmol/L and 116.4 μmol/L, respectively. This indicated that FSPG had a high specificity of binding for the system x_c_−.

In another study, excess concentrations of L-glutamate, L-cysteine, and p-carboxy-phenylglycine (CPG; a specific inhibitor of system x_c_−) were shown to inhibit (~80%) the uptake of [^18^F]FSPG by the NIH-H460 cells (5). However, no such inhibition was observed with D- or L-aspartate. This again indicated that the uptake of [^18^F]FSPG in these cells was specifically mediated through system x_c_−.

A TLC analysis of plasma samples obtained at various time points from mice injected with [^18^F]FSPG showed that the labeled compound remained intact for at least 30 min postinjection (p.i.); later time points were not studied because the tracer was rapidly cleared from circulation (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DFSPG%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]FSPG was investigated in mice bearing NCI-H460 cell tumors (5). The animals (n = 3 mice/time point) were injected with 185 kBq (5 μCi) [^18^F]FSPG through the tail vein, and the rodents were euthanized at time points ranging from 15 min p.i. to 2 h p.i. All organs of interest were obtained from the animals to determine the amount of radioactivity that accumulated in the various tissues (presented as percent of injected dose per gram tissue (% ID/g)). The uptake of label in the tumors was 4.1± 1.4% ID/g at 15 min p.i. and 3.2 ± 0.4% ID/g at 1 h p.i., and it remained relatively constant thereafter. At 1 h p.i., the tumor/blood and tumor/muscle ratios were 14 and 27, respectively. Among all the tissues, the pancreas showed maximum uptake of the tracer (19.4 ± 4.2% ID/g at 15 min p.i., and uptake decreased to 5.8 ± 0.9% ID/g at 1 h p.i.); all other tissues, including the bone, showed <1% ID/g of radioactivity at 15 min p.i. The presence of a low amount of label in the bone indicated that there was no in vivo defluorination of [^18^F]FSPG (5).

A comparative PET imaging study was performed with [^18^F]FSPG and [^18^F]-FDG in nude rats bearing NCI-H460 cell tumors (n = 3 rats/tracer) (5). Identical animal handling and PET imaging protocols were used for both the tracers in this study. The NCI-H460 cell lesions were clearly visible with both [^18^F]FSPG and [^18^F]-FDG; with [^18^F]-FDG, however, high amounts of the label were observed in the muscles, joints, brown fat, and the heart of the animals, in addition to the high levels in the tumor.

Baek et al. evaluated the use of [^18^F]FSPG with PET to detect human Huh7 liver cancer cell orthotropic tumors in the left liver lobe of Naval Medical Research Institute nude mice (n = 3 animals) (8). The rodents were injected with 7.9−8.3 MBq (0.213–0.224 mCi) [^18^F]FSPG (route of injection not reported), and micro-PET images of the mice were acquired at 50 min p.i. for 20 min. A low background signal was observed in the liver and other organs of the animals; besides the tumors, the kidneys, and the bladder, only the pancreas and the thymus showed some uptake of the tracer. At 60 min p.i., the uptake of radioactivity in the tumors was determined to be 4.4 ± 1.3% ID/g, and the tumor/background (T/B) ratio at this time point was 11 ± 1.3.

In another study, the use of [^18^F]FSPG was evaluated with PET to detect hepatoma MH-3924A cell (http://www.cell-lines-service.de/content/e174/e158/e2028/e1412/index_ger.html) tumors in the left liver lobe of August-Copenhagen Irish rats (n = 3 animals) (8). The animals were given 7.9–9.1 MBq (0.213–0.245 mCi) [^18^F]FSPG through an intravenous injection, and micro-PET images of the rats were acquired at 60 min p.i. for 10 min. The pattern of tracer uptake in these animals was similar to that observed in the mouse study described above; the amount of radioactivity accumulated in the tumors was 1.5 ± 0.4% ID/g, and the T/B ratio was 3 ± 2.

From these studies, the investigators concluded that [^18^F]FSPG can probably be used with PET to detect tumors that overexpress the system x_c_− transporter in rodents (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DFSPG%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DFSPG%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DFSPG%20Human%20Studies&cmd=DetailsSearch)]

The use of [^18^F]FSPG was compared with that of [^18^F]FDG for the detection of NSCLC tumors (n = 10 patients) and breast cancer tumors (n = 5 patients) that overexpress system x_c_− in humans (7). For [^18^F]FSPG, each patient was given an intravenous injection of 300 ± 10 MBq (8.1 ± 0.8 mCi; mass dose ≤ 100 μg ) of the tracer, and whole-body PET/computed tomographic (CT) images of the individuals were acquired for different time intervals as described elsewhere (7). For PET/CT imaging with [^18^F]FDG, the patients were given an intravenous injection of 7.4 MBq (0.2 mCi)/kg body weight of the tracer, and whole-body images were acquired as described by Yoon et al. (9). Standardized uptake values (SUV) and the SUV ratios (SUVRs) were calculated from the tumor and blood pool activities as detailed by Baek et al. (7). Using appropriate antibodies, the expression of system x_c_− and CD44 (this antigen stabilizes system x_c_−) in the cancerous lesions of the patients was confirmed with immunohistochemical techniques. In the NSCLC patients, the tumor/blood pool SUVR of [^18^F]FSPG was similar to that obtained with [^18^F]FDG (9.7 ± 8.6 versus 7.7 ± 4.2); however, this ratio was significantly lower (P < 0.05) in the breast cancer patients (3.6 ± 5.4 versus 8.9 ± 7.9). [^18^F]FSPG had sensitivity values of 100% and 60% for the NSCLC tumors (detection of 10out of 10 lesions) and the breast cancer tumors (detection of 3 out of 5 lesions), respectively, among the cancerous lesions confirmed with immunohistochemistry. In addition, with [^18^F]FSPG the SUV of the NSCLC lesions correlated significantly (P < 0.01) with the immunohistochemical stain intensity of system x_c_− transporter and the CD44 antigen. From these studies, the investigators concluded that [^18^F]FSPG may be used with PET to detect neoplastic lesions in the NSCLC patients, and that [^18^F]FSPG can also be used to assess system x_c_− transporter activity in the cancerous lesions (7).

In another study, the use of [^18^F]FSPG was compared with that of [^18^F]FDG for the detection of HCC lesions in the patients of this cancer (8). Five patients with HCC that exhibited hyper- or isometabolic lesions with [^18^F]FDG PET imaging were enrolled to evaluate the tracers. The expression of system x_c_− transporter and the CD44 antigen in the tumors was investigated with immunohistochemistry in 4 out of 5 patients enrolled in the study. The participants were injected with 300 MBq (8.1 mCi) [^18^F]FSPG, and dynamic whole-body PET scans of the patients were acquired for up to 120 min p.i. PET imaging of the patients showed that [^18^F]FSPG and [^18^F]FDG could detect the HCC lesions in 5 out of 5 and 3 out of 5 of the individuals, respectively. Although the SUVRs of tumor/normal liver were comparable for both [^18^F]FSPG and [^18^F]FDG (3.6 ± 2.2 versus 2.7 ± 1.3), the SUV of the healthy liver was significantly lower (P < 0.05) with [^18^F]FSPG than with [^18^F]FDG (1.3 ± 0.3 versus 1.9 ± 0.2). A moderate or intense accumulation of [^18^F]FSPG was observed in two of the patients who showed the expression of system x_c_− and the CD44 antigen in the HCC lesions. Lesions of the other two patients did not show expression of the CD44 antigen and had a low uptake of radioactivity from [^18^F]FSPG. From these studies, the investigators concluded that [^18^F]FSPG may be suitable for the detection of HCC lesions in the clinic (8).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lewerenz J., Hewett S.J., Huang Y., Lambros M., Gout P.W., Kalivas P.W., Massie A., Smolders I., Methner A., Pergande M., Smith S.B., Ganapathy V., Maher P. (2013). The cystine/glutamate antiporter system x(c)(-) in health and disease: from molecular mechanisms to novel therapeutic opportunities. Antioxid Redox Signal.
2 Franco R., Cidlowski J.A. (2012). Glutathione efflux and cell death. Antioxid Redox Signal.
3 Lo M., Wang Y.Z., Gout P.W. (2008). The x(c)- cystine/glutamate antiporter: a potential target for therapy of cancer and other diseases. J Cell Physiol.
4 Lieberman B.P., Ploessl K., Wang L., Qu W., Zha Z., Wise D.R., Chodosh L.A., Belka G., Thompson C.B., Kung H.F. (2011). PET imaging of glutaminolysis in tumors by 18F-(2S,4R)4-fluoroglutamine. J Nucl Med.
5 Koglin N., Mueller A., Berndt M., Schmitt-Willich H., Toschi L., Stephens A.W., Gekeler V., Friebe M., Dinkelborg L.M. (2011). Specific PET imaging of xC- transporter activity using a (1)(8)F-labeled glutamate derivative reveals a dominant pathway in tumor metabolism. Clin Cancer Res.
6 Zhu A., Lee D., Shim H. (2011). Metabolic positron emission tomography imaging in cancer detection and therapy response. Semin Oncol.
7 Baek S., Choi C.M., Ahn S.H., Lee J.W., Gong G., Ryu J.S., Oh S.J., Bacher-Stier C., Fels L., Koglin N., Hultsch C., Schatz C.A., Dinkelborg L.M., Mittra E.S., Gambhir S.S., Moon D.H. (2012). Exploratory clinical trial of (4S)-4-(3-[18F]fluoropropyl)-L-glutamate for imaging xC- transporter using positron emission tomography in patients with non-small cell lung or breast cancer. Clin Cancer Res.
8 Baek S., Mueller A., Lim Y.S., Lee H.C., Lee Y.J., Gong G., Kim J.S., Ryu J.S., Oh S.J., Lee S.J., Bacher-Stier C., Fels L., Koglin N., Schatz C.A., Dinkelborg L.M., Moon D.H. (2013). (4S)-4-(3-18F-fluoropropyl)-L-glutamate for imaging of xC transporter activity in hepatocellular carcinoma using PET: preclinical and exploratory clinical studies. J Nucl Med.
9 Yoon D.H., Baek S., Choi C.M., Lee D.H., Suh C., Ryu J.S., Moon D.H., Lee J.S., Kim S.W. (2011). FDG-PET as a potential tool for selecting patients with advanced non-small cell lung cancer who may be spared maintenance therapy after first-line chemotherapy. Clin Cancer Res.